# Polyethylene glycol-Cys-Arg-Ser-Gly-Pro-Leu-Gly-Val-Tyr-Lys-Lys-tetramethylrhodamine

Chemical name: | Polyethylene glycol-Cys-Arg-Ser-Gly-Pro-Leu-Gly-Val-Tyr-Lys-Lys-tetramethylrhodamine
Abbreviated name: | PEG-peptide-TMR
Synonym: | PEG-CRSGPLGVYKK-TMR
Agent category: | Peptide
Target: | Matrix metalloproteinases (MMPs)
Target category: | Enzyme
Method of detection: | Optical, near-infrared (NIR) fluorescence
Source of signal/contrast: | Tetramethylrohodamine (TMR)
Activation: | Yes
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MMP%20TMR)]

Extracellular matrix (ECM) adhesion molecules consist of a complex network of fibronectins, collagens, chondroitins, laminins, glycoproteins, heparin sulfate, tenascins, and proteoglycans that surround connective tissue cells, and they are mainly secreted by fibroblasts, chondroblasts, and osteoblasts (1). Cell substrate adhesion molecules are considered essential regulators of cell migration, differentiation, and tissue integrity and remodeling. These molecules play a role in inflammation and atherogenesis, but they also participate in the process of invasion and metastasis of malignant cells in the host tissue (2). Tumor cells adhere to the ECM, which provides a matrix environment for the permeation of tumor cells through the basal lamina and underlying interstitial stroma of the connective tissue. Overexpression of matrix metalloproteinases (MMPs) and other proteases by tumor cells allows intravasation of tumor cells into the circulatory system after degrading the basement membrane and ECM (3).

Several families of MMPs are involved in atherogenesis, myocardial infarction, angiogenesis, and tumor invasion and metastases (4-7). MMP expression is highly regulated in normal cells, such as trophoblasts, osteoclasts, neutrophils, and macrophages. Elevated levels of MMPs have been found in tumors associated with a poor prognosis for cancer patients (8). The peptide Gly-Pro-Leu-Gly-Val-Arg-NH_2_ (GPLGVR) was found to be a MMP2/9 substrate and is cleaved between the Gly (G) and Val (V) residues (9). Chuang et al. (10) linked a hydrophilic polyethylene glycol (PEG) group to the N-terminus of Cys-Arg-Ser-Gly-Pro-Leu-Gly-Val-Tyr-Lys-Lys (CRSGPLGVYKK) and a hydrophobic tetramethylrhodamine (TMR) molecule to the C-terminus Lys (K) residue to form PEG-CRSGPLGVYKK-TMR (PEG-peptide-TMR) for optical imaging of protease activity in vivo. Upon MMP cleavage, the lipophilic VYKK-TMR is released and accumulated at the sites (cell surface) of protease activity. The accumulation was most likely attributed to the binding of the lipophilic VYKK-TMR to the cell membrane non-specifically. PEG-peptide-TMR accumulated in HT1080 tumors (with high MMP2 expression) but not in MCF-7 tumors (with low MMP2 expression), as determined with optical imaging in nude mice.

### Related Resource Links:

- Chapters in MICAD (MMP (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=matrix+metalloproteinases+AND+micad%5Bbook%5D))
- Gene information in NCBI (MMP2 (http://www.ncbi.nlm.nih.gov/gene/4313), MMP9 (http://www.ncbi.nlm.nih.gov/gene/4318))
- Articles in Online Mendelian Inheritance in Man (OMIM) (MMP2 (http://omim.org/entry/120360), MMP9 (http://omim.org/entry/120361))
- Clinical trials (MMP (http://www.clinicaltrials.gov/ct2/results?term=matrix+metalloproteinases))
- Drug information in FDA (MMP (http://google2.fda.gov/search?q=matrix+metalloproteinases+&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=10&y=10))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MMP%20TMR)]

A solution of peptide-TMR (available commercially) and methoxy PEG_5000_-maleimide in phosphate-buffered saline (pH 7.4) was incubated for 4 h at room temperature (10). PEG-peptide-TMR was purified with column chromatography with 80%–90% purity. Fluorescence excitation and emission maxima of TMR are 555 nm and 580 nm, respectively. The molecular weight of the PEG-peptide-TMR was confirmed with matrix-assisted laser desorption/ionization-time-of-flight (MALDI-TOF).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MMP%20TMR%20and%20in%20vitro)]

Chuang et al. (10) showed that peptide-TMR (1.618 kDa) was cleaved by purified MMP2 and conditioned medium from MMP-expressing human fibrosarcoma HT1080 cells into two fragments: CRSGPLG (0.670 Da) and VYKK-TMR (0.948 kDa). The cleavage of peptide-TMR was inhibited by a broad-spectrum MMP inhibitor, 1,10-phenanthroline. Conditioned medium from human breast adenocarcinoma MCF-7 cells (with low MMP expression) was unable to cleave peptide-TMR. The reactions were monitored with MALDI-TOF. HT1080 cells or MCF-7 cells were incubated with 5 µM PEG-peptide-TMR for 1 h at 37°C and washed. Fluorescence microscopy and flow cytometry showed that strong fluorescence intensity was observed in HT1080 cells but marginal fluorescence intensity in MCF-7 cells, indicating that VYKK-TMR accumulated in HT1080 cells. Addition of 1,10-phenanthroline to HT1080 cells inhibited the fluorescence intensity by >10-fold. Addition of MMP2 to MCF-7 cells resulted in enhanced fluorescence intensity in MCF-7 cells, indicating VYKK-TMR accumulation and was much less than for HT1080 cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MMP%20TMR%20and%20rodentia)]

Chuang et al. (10) performed in vivo optical imaging studies of PEG-peptide-TMR (35 nmol, intravenously injected) in nude mice (n = 3) bearing HT1080 tumors (high MMP2 expression) and MCF-7 tumors (low MMP2 expression) in their right and left hind legs, respectively. Whole-body optical imaging was performed at 30, 60, and 90 min after injection. Good fluorescence signal was visualized in the HT1080 tumors at 30 min, and the signal reached a maximum at 60 min before declining at 90 min to a signal level near that observed at the 30-min time point. On the other hand, little fluorescence signal was observed in MCF-7 tumors at these time points. Histoimmunological staining of tumor sections revealed strong expression of MMP2 in HT1080 tumors with co-localization of fluorescence signals but not in MCF-7 tumors.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MMP%20TMR%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MMP%20TMR%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MMP%20TMR%20and%20human)]

No publication is currently available.

## References

1 Bosman F.T., Stamenkovic I. (2003). Functional structure and composition of the extracellular matrix. J Pathol.
2 Jiang W.G., Puntis M.C., Hallett M.B. (1994). Molecular and cellular basis of cancer invasion and metastasis: implications for treatment. Br J Surg.
3 Albelda S.M. (1993). Role of integrins and other cell adhesion molecules in tumor progression and metastasis. Lab Invest.
4 Keppler D., Sameni M., Moin K., Mikkelsen T., Diglio C.A., Sloane B.F. (1996). Tumor progression and angiogenesis: cathepsin B & Co. Biochem Cell Biol.
5 Liu J., Sukhova G.K., Sun J.S., Xu W.H., Libby P., Shi G.P. (2004). Lysosomal cysteine proteases in atherosclerosis. Arterioscler Thromb Vasc Biol.
6 Berchem G., Glondu M., Gleizes M., Brouillet J.P., Vignon F., Garcia M., Liaudet-Coopman E. (2002). Cathepsin-D affects multiple tumor progression steps in vivo: proliferation, angiogenesis and apoptosis. Oncogene.
7 Brix, K., A. Dunkhorst, K. Mayer, and S. Jordans, Cysteine cathepsins: Cellular roadmap to different functions. Biochimie, 2007
8 Deryugina E.I., Quigley J.P. (2006). Matrix metalloproteinases and tumor metastasis. Cancer Metastasis Rev.
9 Bae M., Cho S., Song J., Lee G.Y., Kim K., Yang J., Cho K., Kim S.Y., Byun Y. (2003). Metalloprotease-specific poly(ethylene glycol) methyl ether-peptide-doxorubicin conjugate for targeting anticancer drug delivery based on angiogenesis. Drugs Exp Clin Res.
10 Chuang C.H., Chuang K.H., Wang H.E., Roffler S.R., Shiea J.T., Tzou S.C., Cheng T.C., Kao C.H., Wu S.Y., Tseng W.L., Cheng C.M., Hou M.F., Wang J.M., Cheng T.L. (2012). In Vivo Positron Emission Tomography Imaging of Protease Activity by Generation of a Hydrophobic Product from a Noninhibitory Protease Substrate. Clin Cancer Res.